# ^124^I-Anti–prostate stem-cell antigen back-mutated 2B3 diabody

Chemical name: | ^124^I-Anti–prostate stem-cell antigen back-mutated 2B3 diabody
Abbreviated name: | ^124^I-bm2B3-Db8
Synonym:
Agent category: | Antibody
Target: | Prostate stem-cell antigen (PSCA)
Target category: | Antigen
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^124^I
Activation: | No
Studies: | - In Vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=2909844), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=9367211) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=8000) for more information about PSCA.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=2B3%20minibody)]

Prostate stem-cell antigen (PSCA) is a cell-surface protein (123 amino acids) that is expressed in normal prostate tissue and overexpressed in prostate cancer tissues (1). PSCA expression is detected in >80% of patients with local disease, including high expression in bone metastases (2). Elevated levels of PSCA are correlated with increased tumor stage, grade, and androgen independence (3). PSCA overexpression is also observed in bladder and pancreatic cancers (4).

The anti-PSCA murine monoclonal antibody (mAb) 1G8 has been shown to have anti-tumor activity (5). A humanized version of the 1G8 mAb (hu1G8) has been radiolabeled as ^124^I-hu1G8 for tumor imaging in mice (6). However, it took ~1 week to observe an enhanced target/background ratio with positron emission tomography (PET) because of the slow kinetics of the mAb. A hu1G8 minibody fragment (2B3), a dimer of scFvs-C_H_3 with a linker composed of 18 amino acids (molecular weight, ~80 kDa), has been developed and labeled as ^124^I-2B3 minibody for tumor-targeting studies (7). To create a stable, rapidly clearing antibody fragment, the parental 2B3 diabody (p2B3-Db) (molecular weight, 55 kDa) was mutated back to the original mouse residues to produce a high-affinity, back-mutated diabody with a linker of 8 amino acids (bm2B3-Db8) (8). ^124^I-p2B3-Db8 and ^124^I-bm2B3-Db8 were evaluated for tumor imaging.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=2B3%5BAll+Fields%5D+AND+micad%5Bbook%5D)
- Gene information in NCBI (PSCA (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=DetailsSearch&Term=8000%5Buid%5D))
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/entrez/dispomim.cgi?id=602470)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=124I+AND+2B3+synthesis)]

The p2B3-Db8 and bm2B3-Db8 diabodies were labeled with [^124^I]sodium iodide by the Iodogen method (8). ^124^I-p2B3-Db8 and ^124^I-bm2B3-Db8 were purified with gel filtration, and each labeled diabody exhibited a specific activity of ~5.6 MBq/nmol (0.15 mCi/nmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=124I+2B3+and+in+vitro)]

With the use of PSCA competition assays, binding affinity (K_d_) values were found to be 5.4 nM for p2B3-Db8, 1.9 nM for bm2B3-Db8, and 46 nM for 2B3 minibody (8).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=124I+2B3+and+rodentia)]

Leyton et al. (8) performed biodistribution studies with ^124^I-p2B3-Db8 and ^124^I-bm2B3-Db8 (~0.6 nmol/mouse) in nude mice bearing xenografts of the LAPC-9 (PSCA-positive) and PC-3 (PSCA-negative) tumor cell lines. The ^124^I-bm2B3-Db8 uptake in the LAPC tumors was 1.02 ± 0.2% injected dose per gram (% ID/g) at 20 h after injection, whereas the uptake in the PC-3 tumors was 0.51 ± 0.1% ID/g. Accumulation of radioactivity in the lung, liver, spleen, and kidney was lower than in the LAPC-9 tumor. Accumulation in the thyroid and stomach was not reported. The tumor/blood and tumor/control tumor ratios were 1.2 and 2.0, respectively. On the other hand, the ^124^I-p2B3-Db8 uptake was 0.57 ± 0.2% ID/g in the LAPC tumors and 0.34 ± 0.2% ID/g in the PC-3 tumors. The tumor/blood and tumor/control tumor ratios were 0.7 and 1.7, respectively. The tumor accumulation of ^124^I-bm2B3-Db8 was lower than that of ^124^I-2B3 minibody in the same tumor model as reported previously (7). PET imaging with ^124^I-bm2B3-Db8 visualized the LAPC-9 tumor as early as 4 h after injection with a higher contrast at 12 h. No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=124I+2B3+and+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=124I+2B3+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=124I+2B3+and+human)]

No publication is currently available.

## NIH Support

CA92131, CA86306, P01 CA43904, CA16042

## References

1 Reiter R.E., Gu Z., Watabe T., Thomas G., Szigeti K., Davis E., Wahl M., Nisitani S., Yamashiro J., Le Beau M.M., Loda M., Witte O.N. (1998). Prostate stem cell antigen: a cell surface marker overexpressed in prostate cancer. Proc Natl Acad Sci U S A.
2 Lam J.S., Yamashiro J., Shintaku I.P., Vessella R.L., Jenkins R.B., Horvath S., Said J.W., Reiter R.E. (2005). Prostate stem cell antigen is overexpressed in prostate cancer metastases. Clin Cancer Res.
3 Gu Z., Thomas G., Yamashiro J., Shintaku I.P., Dorey F., Raitano A., Witte O.N., Said J.W., Loda M., Reiter R.E. (2000). Prostate stem cell antigen (PSCA) expression increases with high gleason score, advanced stage and bone metastasis in prostate cancer. Oncogene.
4 Amara N., Palapattu G.S., Schrage M., Gu Z., Thomas G.V., Dorey F., Said J., Reiter R.E. (2001). Prostate stem cell antigen is overexpressed in human transitional cell carcinoma. Cancer Res.
5 Gu Z., Yamashiro J., Kono E., Reiter R.E. (2005). Anti-prostate stem cell antigen monoclonal antibody 1G8 induces cell death in vitro and inhibits tumor growth in vivo via a Fc-independent mechanism. Cancer Res.
6 Olafsen T., Gu Z., Sherman M.A., Leyton J.V., Witkosky M.E., Shively J.E., Raubitschek A.A., Morrison S.L., Wu A.M., Reiter R.E. (2007). Targeting, imaging, and therapy using a humanized antiprostate stem cell antigen (PSCA) antibody. J Immunother.
7 Leyton J.V., Olafsen T., Lepin E.J., Hahm S., Bauer K.B., Reiter R.E., Wu A.M. (2008). Humanized radioiodinated minibody for imaging of prostate stem cell antigen-expressing tumors. Clin Cancer Res.
8 Leyton J.V., Olafsen T., Sherman M.A., Bauer K.B., Aghajanian P., Reiter R.E., Wu A.M. (2009). Engineered humanized diabodies for microPET imaging of prostate stem cell antigen-expressing tumors. Protein Eng Des Sel.